# Cy5.5-Knottin 2.5D

Chemical name: | Cy5.5-Knottin 2.5D
Abbreviated name: | Cy5.5-Knottin 2.5D
Synonym:
Agent Category: | Ligand
Target: | α_v_β_3_, α_v_β_5_, and α_5_β_1_ integrin receptors
Target Category: | Receptors
Method of detection: | Near-infrared fluorescence
Source of signal / contrast: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=knottin+peptides)]

Integrin receptors that mediate tumor angiogenesis, growth, and metastasis through a complex network of signaling pathways are known to be expressed on the surface of cancerous tumor cells and neovasculature (1-3). Because of their role in tumor development and progression, inhibition of integrin receptor activity is being actively investigated in clinical trials for the treatment (http://clinicaltrials.gov/ct2/results?term=integrin+inhibitors) and imaging (http://clinicaltrials.gov/ct2/results?term=integrin+imaging) of various cancers (4, 5). Non-invasive imaging probes can be used to determine not only the efficacy of integrin-targeted anti-cancer drugs, but also to monitor disease progression and metastasis (6, 7). Although integrin receptors usually bind through the arginine-glycine-aspartic acid (RGD) motif of the extracellular matrix protein ligands, it is the amino acid residues surrounding the RGD motif that determine the receptor specificity and affinity for the ligand (4, 8, 9). As a result of the small size of the drugs, mainly peptides, that target the integrin receptor, it has been challenging to generate peptides containing the RGD motif that have an improved pharmacokinetic behavior, receptor affinity, and tumor uptake for in vivo imaging purposes. Any modification of the peptide structure has yielded integrin-targeted imaging agents that have only a limited advancement and application in the clinics (10, 11). Only one imaging compound with an RGD motif, a radioactive fluorine-labeled cyclic pentapeptide ([^18^F]-galacto-RGD), was determined to be suitable to identify integrin-positive tumors and to investigate α_v_β_3_ integrin expression in humans. However, [^18^F]-galacto-RGD has been shown to have a low tumor uptake, and it generated a high background signal due to accumulation in the liver (12, 13).

In an effort to develop imaging agents for the detection of integrin receptors expressed on tumor cell surface and neovasculature, Kimura et al. (14) used the directed evolution technique (15, 16) to place the integrin-binding RGD motif into a cystine knot peptide (also known as knottins) trypsin inhibitor of the squash plant (Ecballium elaterium) (17). The peptide was reported to have a high affinity for the α_v_β_3_ and α_v_β_5_ or the α_v_β_3_, α_v_β_5_, and α_5_β_1_ integrin receptors. In general, knottins have a core structure containing a disulfide bond, are resistant to proteolysis, have a high thermodynamic stability, and are nonimmunogenic (14). The knottin peptide containing an RGD motif (designated as knottin 2.5D) was labeled with Cy5.5, a near-infrared (NIR) fluorescent cyanine dye, to obtain Cy5.5-knottin 2.5D, and the Cy5.5 conjugate was used to image integrin-expressing xenograft tumors in mice with NIR fluorescence imaging. It is pertinent to mention that the knottin 2.5D discussed in this chapter and the knottin 2.5F peptide discussed separately in MICAD (www.micad.nih.gov) were developed and investigated by Kimura et al. (14). The structural and amino acid sequence similarities and differences of the two peptides have been described elsewhere (14).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu+knottin+2%2E5D+synthesis)]

The synthesis of knottin 2.5D was performed with the use of the 9-fluorenylmethylcarbonyl-based solid-phase technique as described by Kimura et al. (14). In addition, two other knottin peptides, FN-RGD2 (for use as positive a control) and FN-RDG2 (negative control) were synthesized using the same technique mentioned above. A third peptide, c(RGDyK), was obtained from commercial sources for use as a second control. The amino acid sequence, structure, and properties of the various integrin-binding peptides used for studies described in this chapter are discussed by Kimura et al. (14).

To conjugate knottin 2.5D to Cy5.5, the knottin was mixed with a solution of Cy5.5-N-hydroxysuccinimide ester in dimethylsulfoxide and triethylamine. The reaction was allowed to proceed at room temperature in the dark (duration not reported) with constant monitoring with reverse-phase high-performance liquid chromatography (RP-HPLC) on a C_18_ column (14). Upon completion of the reaction, the conjugated peptide was purified with semi-preparative RP-HPLC and freeze-dried for storage (conditions not reported). The peptide purity and molecular mass were respectively confirmed with analytical RP-HPLC and electrospray or matrix-assisted laser desorption/ionization time-of-flight mass spectrometery. Yield of the final product, the number of Cy5.5 molecules conjugated to each molecule of knottin 2.5D, and the stability of the fluorescent dye–labeled knottin were not reported.

Echistatin labeled with radioactive iodine (^125^I-echistatin), used as a control in some studies, was obtained from a commercial source (14).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu+knottin+2%2E5D+in+vitro+studies)]

To determine the relative integrin-binding affinities (reported as 50% inhibitory concentration (IC_50_)) of the modified and unmodified peptides, including knottin 2.5D, a competition binding assay was performed with ^125^I-echistatin (a strong antagonist of α_v_β_3_, α_v_β_5_, α_5_β_1_ and α_iib_β_3_ integrins (14)) using U-87MG cells (a human glioblastoma cell line that expresses several types of integrins on the cell surface) as described by Kimura et al. (14). The IC_50_ for Cy5.5-knottin 2.5D was determined to be 4.8 ± 1.1 nmol/L compared with IC_50_ values of 19 ± 6 nmol/L, 370 ± 150 nmol/L, and 860 ± 400 nmol/L for the control unconjugated knottin 2.5D, FN-RGD2, and c(RGDyK) peptides, respectively. The negative control FN-RDG2 peptide, with or without Cy5.5 conjugation, did not compete with ^125^I-echistatin for binding to the U-87MG cells (14).

The integrin-binding specificity of Cy5.5-knottin 2.5D was investigated with a competition displacement assay using imobalized intergrin receptors and ^125^I-echistatin (14). Different concentrations (5 and 50 nmol/L) of the conjugated knottin 2.5D and the control peptides were respectively incubated with ^125^I-echistatin in microtiter plates coated with detergent-solubalized α_v_β_3_, α_v_β_5_, α_5_β_1_, and α_iib_β_3_ integrin receptors for 3 h at room temperature. The plates were washed three times to remove unbound radioactivity, and the contents were solubalized in 2 N sodium hydroxide to determine the amount of receptor-bound radioactivity. Compared with the conjugated FN-RGD2 and c(RGDyK) peptides, the Cy5.5-knottin 2.5D peptide exhibited a high competition for ^125^I-echistatin binding to the different integrin receptors (varying from ~35 to 95% reduction in binding of labeled echistatin using a low (5nmol/L) and a high (50 nmol/L) concentration of the unlabeled peptides) except the α_iib_β_3_ receptor, which is expressed mainly on blood platelet cells (14).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu+knottin+2%2E5D+rodentia)]

The use of Cy5.5-knottin 2.5D as an NIR imaging probe was investigated in mice bearing human U-87MG cell xenograft tumors and compared with imaging results obtained with the Cy5.5-conjugated control peptides (14). The animals (n = 3 mice for each probe) were injected with the respective Cy5.5-conjugated peptides through the tail vein and imaged at various time points up to 24 h. Whole-body imaging was performed on the animals, and the tumor/normal tissue fluorescence ratios (T/N) were calculated. The T/N ratios (for details see Figure 3B in reference 14) generated with Cy5.5-knottin 2.5D had a low standard deviation (~2.5 at 1 h and ~4.5 at 24 h) and were significantly (P < 0.05) higher than those obtained from the control Cy5.5-conjugated peptides (~2.2 at 1 h and ~3.0 at 24 h) at all time points from 0 to 24 h after administration of the probes. Also, the signal obtained with the positive control Cy5.5-conjugated peptides was only slightly higher than that of the negative control, FN-RDG2 peptide (~2 at 1 h and 2.5 at 24 h). No in vivo biodistribution of the Cy5.5-conjugated knottin 2.5D peptide was reported.

From these studies the investigators concluded that the direct evolution–engineered integrin-binding peptides are probably suitable for the detection and diagnosis of various cancers (14).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu+knottin+2%2E5D+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu+knottin+2%2E5D+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## NIH Support

Some of the work presented in this chapter was supported by National Cancer Institute grants 5K01 CA104706, 5R25T CA118681, and R25T CA118681 and a National Institutes of Health grant P50 CA114747.

## References

1 Legate K.R., Wickstrom S.A., Fassler R. (2009). Genetic and cell biological analysis of integrin outside-in signaling. Genes Dev.
2 Pontier S.M., Muller W.J. (2009). Integrins in mammary-stem-cell biology and breast-cancer progression--a role in cancer stem cells?. J Cell Sci.
3 Streuli C.H. (2009). Integrins and cell-fate determination. J Cell Sci.
4 Moschos S.J., Drogowski L.M., Reppert S.L., Kirkwood J.M. (2007). Integrins and cancer. Oncology.
5 Fujita Y., Abe R., Shimizu H. (2008). Clinical approaches toward tumor angiogenesis: past, present and future. Curr Pharm Des.
6 Zaccaro L., Del Gatto A., Pedone C., Saviano M. (2009). Peptides for tumour therapy and diagnosis: current status and future directions. Curr Med Chem.
7 Haubner R., Decristoforo C. (2009). Radiolabelled RGD peptides and peptidomimetics for tumour targeting. Front Biosci.
8 Chen, C.Y., J.H. Shiu, Y.H. Hsieh, Y.C. Liu, Y.C. Chen, Y.C. Chen, W.Y. Jeng, M.J. Tang, S.J. Lo, and W.J. Chuang, Effect of D to E mutation of the RGD motif in rhodostomin on its activity, structure, and dynamics: Importance of the interactions between the D residue and integrin. Proteins, 2009
9 Manzoni, L., L. Belvisi, D. Arosio, M. Civera, M. Pilkington-Miksa, D. Potenza, A. Caprini, E.M. Araldi, E. Monferini, M. Mancino, F. Podesta, and C. Scolastico, Cyclic RGD-Containing Functionalized Azabicycloalkane Peptides as Potent Integrin Antagonists for Tumor Targeting. ChemMedChem, 2009
10 Cai W., Rao J., Gambhir S.S., Chen X. (2006). How molecular imaging is speeding up antiangiogenic drug development. Mol Cancer Ther.
11 Haubner R. (2006). Alphavbeta3-integrin imaging: a new approach to characterise angiogenesis?. Eur J Nucl Med Mol Imaging.
12 Haubner R., Weber W.A., Beer A.J., Vabuliene E., Reim D., Sarbia M., Becker K.F., Goebel M., Hein R., Wester H.J., Kessler H., Schwaiger M. (2005). Noninvasive visualization of the activated alphavbeta3 integrin in cancer patients by positron emission tomography and [18F]Galacto-RGD. PLoS Med.
13 Beer A.J., Haubner R., Sarbia M., Goebel M., Luderschmidt S., Grosu A.L., Schnell O., Niemeyer M., Kessler H., Wester H.J., Weber W.A., Schwaiger M. (2006). Positron emission tomography using [18F]Galacto-RGD identifies the level of integrin alpha(v)beta3 expression in man. Clin Cancer Res.
14 Kimura R.H., Cheng Z., Gambhir S.S., Cochran J.R. (2009). Engineered knottin peptides: a new class of agents for imaging integrin expression in living subjects. Cancer Res.
15 Otten L.G., Quax W.J. (2005). Directed evolution: selecting today's biocatalysts. Biomol Eng.
16 Leemhuis H., Kelly R.M., Dijkhuizen L. (2009). Directed evolution of enzymes: Library screening strategies. IUBMB Life.
17 Favel A., Mattras H., Coletti-Previero M.A., Zwilling R., Robinson E.A., Castro B. (1989). Protease inhibitors from Ecballium elaterium seeds. Int J Pept Protein Res.